# ^89^Zr-Desferrioxamine B-Transferrin

Chemical name: | ^89^Zr-Desferrioxamine B-Transferrin
Abbreviated name: | ^89^Zr-DFO-Transferrin, ^89^Zr-Transferrin, ^89^Zr-TF
Synonym:
Agent category: | Polypeptide
Target: | Transferrin receptor (TFRC, CD71, p90)
Target category: | Receptor
Method of detection: | Positron emission tomography
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAH01188.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_003234.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/7037) for more information about transferrin receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin)]

Transferrin (TF) is part of a family of proteins that includes serum TF, ovotransferrin, and lactoferrin (1). Serum TF is a monomeric glycoprotein (molecular mass, 76.5 kDa) that binds two Fe^3+^ ions for delivery to cells through receptor-mediated endocytosis. TF is mainly produced in the liver, but other tissues and organs also produce it. The TF receptor (TFRC) mediates the internalization of iron-loaded TF into cells (1, 2). Iron usage is required for various biological processes associated with cell proliferation. The TFRC (CD71 or p90) is a type II transmembrane glycoprotein and is found primarily as a homodimer (molecular mass, 180 kDa). It also contains other growth regulatory functions in certain normal and malignant cells. Overexpression of TFRC in cancer cells can be linked to upregulation of transcription factors, such as MYC (an oncogene protein) (3) and HIF-1α (a hypoxia factor) (4). The elevated levels of TFRC in some malignancies (e.g., 74% breast carcinomas, 76% lung adenocarcinomas, and 93% lung squamous cell carcinomas) and the extracellular accessibility of this molecule make TFRC a potential molecular target for cancer imaging or therapy (1, 2). Activated leukocytes also have elevated expression of TFRC. Holland et al. (5) prepared ^89^Zr-N-succinyldesferrioxamine B-transferrin (^89^Zr-DFO-transferrin, ^89^Zr-TF) for imaging TFRC expression in inflamed tissue in mice, in MYC prostate cancer (MycCap) cells in transgenic mice, and in MycCap xenografts in mice. Evans et al. (6) evaluated ^89^Zr-TF for use in imaging tumor burden in the brain.

### Related Resource Links:

- Chapters in MICAD (transferrin (http://www.ncbi.nlm.nih.gov/books/?term=transferrin+AND+micad%5Bbook%5D))
- Gene information in NCBI (TFRC (http://www.ncbi.nlm.nih.gov/gene/7037), transferrin (http://www.ncbi.nlm.nih.gov/gene/7018))
- Articles in Online Mendelian Inheritance in Man (OMIM) (TFRC (http://omim.org/entry/190010), transferrin (http://omim.org/entry/190000))
- Clinical trials (transferrin (http://www.clinicaltrials.gov/ct2/results?term=transferrin))
- Drug information in FDA (transferrin (http://google2.fda.gov/search?q=transferrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin+synthesis)]

DFO-TF was prepared by mixing mouse apo-TF (apo – no Fe^3+^) with four molar equivalents of Fe(N-succinyldesferrioxamine B-tetrafluorophenol) in buffer (pH 3.9) (5). Then an excess of ethylenediamine tetraacetic acid was added to the mixture and incubated for 60 min at 38°C. DFO-Conjugated mouse apo-TF (DFO-mTF) was purified with column chromatography. ^89^Zr-Oxalate (380 MBq, 10.3 mCi) in 1.0 M oxalic acid (pH ~8.0) was added to 12 nmol DFO-mTF in saline and incubated for 1–2 h at room temperature. ^89^Zr-mTF was isolated with spin-column centrifugation with >99% radiochemical purity, >80% radiochemical yield, and a specific activity of 27.6 ± 1.0 MBq/nmol (0.75 ± 0.03 mCi/nmol) (n = 7). ^89^Zr-DFO-human TF (^89^Zr-hTF) and ^89^Zr-DFO-mouse albumin (^89^Zr-mAlb) were prepared similarly, with specific activities of 16.5 ± 0.4 MBq/nmol (0.45 ± 0.01 mCi/nmol) (n = 3) and 10.7 ± 0.3 MBq/nmol (0.29 ± 0.01 mCi/nmol) (n = 4), respectively. There were ~2 moieties of DFO per protein conjugate as determined with isotopic dilution assays. ^89^Zr-mTF, ^89^Zr-hTF, and ^89^Zr-mAlb were >98% intact after incubation in saline for 5 d at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin+in+vitro)]

In vitro cellular uptake assays were performed in mouse MycCap and human HeLa cells with ^89^Zr-mTF and ^89^Zr-hTF (5), respectively. The cellular uptake values in MycCap cells were 2% and 24% with ^89^Zr-mTF (apo – no Fe^3+^) and ^89^Zr-mTF (holo with Fe^3+^), respectively. On the other hand, cellular uptake values in HeLa were 13% and 54% with ^89^Zr-hTF (apo – no Fe^3+^) and ^89^Zr-hTF (holo with Fe^3+^), respectively. The holo forms of ^89^Zr-mTF and ^89^Zr-hTF were internalized 11- and 3-fold more than their respective apo forms.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin+rodentia)]

Holland et al. (5) performed PET imaging of inflammation in mice treated with turpentine oil in the right hind limb at 1, 5, and 24 h after intravenous injection of 1.85 MBq (0.05 mCi) ^89^Zr-mTF (n = 5), ^89^Zr-hTF (n = 5), or ^89^Zr-mAlb (n = 2). ^89^Zr-mTF and ^89^Zr-hTF localized to the inflamed tissue within 1 h and persisted over 24 h. The radioactivity in the inflamed tissue at 24 h was 6.5 ± 0.3% injected dose (ID/g) for ^89^Zr-mTF and ^89^Zr-hTF, and 0.8% ID/g for ^89^Zr-mAlb. The radioactivity levels for the contralateral limb were 0.8 ± 0.1% for the three tracers. The inflamed/control ratios were 8.1 ± 0.4 for ^89^Zr-mTF and ^89^Zr-hTF, and 1.0 for ^89^Zr-mAlb, whereas the inflamed/control ratio for [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) was 1.7 ± 0.3 with inflamed tissue radioactivity of 3.7 ± 0.9% ID/g (n = 5). The liver, heart, and kidneys are also visualized with the three tracers. Ex vivo biodistribution studies at 24 h after injection of ^89^Zr-mTF (n = 5), ^89^Zr-hTF (n = 5), and ^89^Zr-mAlb (n = 2) confirmed the PET imaging results with inflamed/control ratios of 6.6 ± 1.9, 6.7 ± 2.9, and 0.9 ± 0.2, respectively. The findings are consistent with increased TFRC expression on activated leukocytes in the inflamed tissue. No blocking studies were performed.

Ex vivo biodistribution studies were performed in male mice (n = 4/group) transplanted with MycCap tumors after injection of 0.74 MBq (0.02 mCi) ^89^Zr-mTF at 1, 5, and 24 h (5). Accumulation of radioactivity in the tumors was 0.88% injected dose/gram (ID/g) at 1 h and increased to 3.14% ID/g and 3.24% ID/g at 5 h and 24 h, respectively. Accumulation (>4% ID/g) in the normal tissues, such as the blood, heart, lung, gastrointestinal tract, liver, and kidney, was higher than in the tumors. On the other hand, radioactivity in the spleen, pancreas, stomach, intestines, testes, muscle, and bone (0.73%–2.65% ID/g) was less than in the tumors. PET imaging and ex vivo studies showed that radioactivity accumulation of ^89^Zr-mTF in the MycCap tumors was 2-fold lower in the castrated male mice versus in the intact hosts at 5 h and 24 h (P < 0.001). No blocking studies were performed.

Further ^89^Zr-mTF PET imaging and ex vivo studies were performed in Hi-Myc transgenic mice (n = 7), which develop invasive prostate adenocarcinoma by 1 yr of age (5). PET imaging data showed tumor radioactivity accumulation of 4.3 ± 0.2% ID/g at 24 h after injection of ~12 MBq (0.32 mCi) ^89^Zr-mTF and a tumor/background contrast ratio of 7.3 ± 1.7. No contrast was observed in the prostate of the wild-type mice (n = 3). High doses of holo mTF (200 mg/kg) administered 45 min before ^89^Zr-mTF injection in Hi-Myc transgenic mice (n = 4) reduced the radioactivity in the prostate by 50% at 24 h. Ex vivo PET imaging and biodistribution studies confirmed the specific accumulation in the prostate of Hi-Myc mice.

Evans et al. (6) showed high radioactivity accumulation (~15% ID/g at 24 h) in TS543 human glioblastomas transplanted subcutaneously in nude mice (n = 5/group) as measured with PET and ex vivo biodistribution studies after intravenous injection of ^89^Zr-hTF at 1–48 h. The maximum tumor/muscle and tumor/brain ratios at 24 h were 7 and 50, respectively. Using the same tumor model, [^18^F]FDG showed a tumor/brain ratio of 1. Whole-brain PET imaging studies were performed in nude mice (n = 4) inoculated with TS543 tumor cells via an intracranial injection into the right brain after intravenous injection of ^89^Zr-hTF. The orthotropic tumors were clearly visualized at 24 h, whereas no contrast was observed in the brains of mice receiving a sham injection. Ex vivo biodistribution data (at 24 h) confirmed the PET imaging with 2.6-fold higher radioactivity accumulation in the orthotropic tumors (1.7 ± 1.0% ID/g) than in the normal left brain (0.5 ± 0.4% ID/g). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr%20transferrin+human)]

No publication is currently available.

## NIH Support

R24 CA83084, R25 CA 096945, P30 CA08748, P50 CA92629

## References

1 Daniels T.R., Delgado T., Rodriguez J.A., Helguera G., Penichet M.L. (2006). The transferrin receptor part I: Biology and targeting with cytotoxic antibodies for the treatment of cancer. Clin Immunol.
2 Daniels T.R., Delgado T., Helguera G., Penichet M.L. (2006). The transferrin receptor part II: targeted delivery of therapeutic agents into cancer cells. Clin Immunol.
3 O'Donnell K.A., Yu D., Zeller K.I., Kim J.W., Racke F., Thomas-Tikhonenko A., Dang C.V. (2006). Activation of transferrin receptor 1 by c-Myc enhances cellular proliferation and tumorigenesis. Mol Cell Biol.
4 Tacchini L., Bianchi L., Bernelli-Zazzera A., Cairo G. (1999). Transferrin receptor induction by hypoxia. HIF-1-mediated transcriptional activation and cell-specific post-transcriptional regulation. J Biol Chem.
5 Holland J.P., Evans M.J., Rice S.L., Wongvipat J., Sawyers C.L., Lewis J.S. (2012). Annotating MYC status with 89Zr-transferrin imaging. Nat Med.
6 Evans M.J., Holland J.P., Rice S.L., Doran M.G., Cheal S.M., Campos C., Carlin S.D., Mellinghoff I.K., Sawyers C.L., Lewis J.S. (2013). Imaging tumor burden in the brain with 89Zr-transferrin. J Nucl Med.